# ^99m^Tc-Galactosyl-methylated chitosan

Chemical name: | ^99m^Tc-Galactosyl-methylated chitosan
Abbreviated name: | ^99m^Tc-GMC
Synonym:
Agent category: | Compound
Target: | Asialoglycoprotein receptors (ASGP-Rs)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4502251), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/186910312) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=432) for more information about ASGP-R.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC)]

Asialoglycoprotein (ASGP) is specifically taken into mammalian hepatocytes by binding to ASGP receptors (ASGP-Rs) (1). The galactosyl moiety of ASGP is recognized on the surface of hepatocytes and is bound by ASGP-R. The ASGP–ASGP-R complex on the cell surface is subsequently taken into cytoplasm by endocytosis and transferred to lysosomes. ASGP-R is then dissociated from ASGP and recycled to the cell surface. ASGP is degraded in the lysosomes and excreted into the bile. The number of ASGP-Rs on the hepatocytes of individuals with liver disease decreases and is thus considered a good indicator for the evaluation of liver function. Because ASGP-R recognizes galactose, ^99m^Tc-diethylenetriamine pentaacetic acid-galactosyl-human serum albumin (^99m^Tc-GSA) (2, 3) and ^99m^Tc-galactosyl-neoglycoalbumin (^99m^Tc-NGA) (4) are ASGP-R probes that accumulate specifically in the liver and are used for liver scintigraphy to determine liver mass and function. Chitosan is a linear polysaccharide composed of D-glucosamine and N-acetylglucosamine subunits with numerous amine groups of D-glucosamine for ligand conjugation. Kim et al. (5) conjugated galactose (via lactobionic acid) to methylated chitosan for radiolabeling with ^99m^Tc to form ^99m^Tc-galactosyl-methylated chitosan (^99m^Tc-GMC) for imaging ASGP-R expression in the liver.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+synthesis)]

Deacetylated chitosan (5 kDa) was incubated with lactobionic acid, 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide hydrochloride, and N-hydroxysuccinimide for 72 h at room temperature (5). The resulting galactosylated chitosan was purified with dialysis and incubated with excess methyl iodide in the presence of sodium hydroxide for 1 h at ~60°C. GMC was isolated by precipitation with ethanol and centrifugation. GMC was incubated with 111 MBq (3 mCi) ^99m^Tc-sodium pertechnetate, tricine, and stannous chloride for 30 min at room temperature. ^99m^Tc-GMC conjugates were prepared with a labeling efficiency of >95%. ^99m^Tc-GMC conjugates were stable in saline up to 6 h. The stability in human serum was >81% up to 2 h. The amount of galactose in galactosylated chitosan was 7.5 mol%. The composition of tri-, di-, and mono-methylation was 9, 46, and 35 mol%, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+in+vitro)]

No publication is currently available

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+rodentia)]

Kim et al. (5) performed ex vivo biodistribution studies in normal mice (n = 5/group) after intravenous injection of ^99m^Tc-GMC at 10, 60, and 120 min. The initial tracer accumulation in the liver was 11.2% injected dose per gram (ID/g) at 10 min, 14.0% ID/g at 60 min, and 14.1% ID/g at 120 min after injection. The kidneys had the highest accumulation with 27.3%, 22.0%, and 19.6% ID/g at these time points, respectively. ^99m^Tc-GMC was largely cleared by the kidneys. The stomach, intestine, heart, lung, muscle, blood, and spleen all showed relatively low accumulation (<4% ID/g). Single-photon emission computed tomography scintigraphic imaging was performed in mice after intravenous injection of 18.5 MBq (0.5 mCi) ^99m^Tc-GMC at 10, 30, 60, and 120 min after injection. High accumulation was observed in the liver and kidneys within a few minutes after injection. The urinary bladder was also highly visualized. Injection of ^99m^Tc-methylated chitosan (non-galactosylated) showed high accumulation in the kidneys and urinary bladder with low radioactivity in the liver. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20HGC+human)]

No publication is currently available.

## References

1 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
2 Kwon A.H., Ha-Kawa S.K., Uetsuji S., Kamiyama Y., Tanaka Y. (1995). Use of technetium 99m diethylenetriamine-pentaacetic acid-galactosyl-human serum albumin liver scintigraphy in the evaluation of preoperative and postoperative hepatic functional reserve for hepatectomy. Surgery.
3 Wu J., Ishikawa N., Takeda T., Tanaka Y., Pan X.Q., Sato M., Todoroki T., Hatakeyama R., Itai Y. (1995). The functional hepatic volume assessed by 99mTc-GSA hepatic scintigraphy. Ann Nucl Med.
4 Vera D.R., Stadalnik R.C., Krohn K.A. (1985). Technetium-99m galactosyl-neoglycoalbumin: preparation and preclinical studies. J Nucl Med.
5 Kim E.M., Jeong H.J., Park I.K., Cho C.S., Kim C.G., Bom H.S. (2005). Hepatocyte-targeted nuclear imaging using 99mTc-galactosylated chitosan: conjugation, targeting, and biodistribution. J Nucl Med.